# ^111^In-CHX-A”-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^111^In-CHX-A”-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^111^In-CHX-A”-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC1) receptor (MC1R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily, and these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and the pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via MC1R.

Positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) in cancer has been approved by United States Food and Drug Administration with many on-going clinical trials. Although [^18^F]FDG is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). N-(2-Aminoethyl)-trans-1,2-diaminocyclohexane-N,N”,N”’-pentaacetic acid (CHX-A”) has been successfully coupled to α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7, 11, 12). A rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (ReCCMSH(Arg^11^)), was conjugated with CHX-A” (CHX-A”-ReCCMSH(Arg^11^)) and radiolabeled with ^111^In (^111^In-CHX-A”-ReCCMSH(Arg^11^)) as a molecular imaging agent for single-photon emission computed tomography (SPECT) to target melanoma (13). Rhenium-mediated cyclization exhibits significantly reduced nonspecific renal radioactivity accumulation, high tumor uptake and retention coupled with rapid clearance kinetics, compared with its free sulfhydryl and disulfide bond–containing counterparts (10). ^111^In is a gamma emitter with a physical half-life of 2.8 days.

### Related Resource Links:

- Chapters in MICAD (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MSH+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157))
- Articles in OMIM (MC1R (http://omim.org/entry/155555))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+and+synthesis)]

Wei et al. (13) reported the synthesis of ^111^In-CHX-A”-ReCCMSH(Arg^11^). The CCMSH(Arg^11^) peptide was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. CCMSH(Arg^11^) was then reacted with 2 M excess of the glutaric acid succinimidyl ester derivative of CHX-A” to the N-terminus of CCMSH(Arg^11^) to form CHX-A”-CCMSH(Arg^11^). A mixture of CHX-A”-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated for 30 min at 85°C. The cyclized peptide, CHX-A”-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography (HPLC). For ^111^In labeling, a solution of 44.4 MBq (1.2 mCi) ^111^InCl_3_ and 10 nmol CHX-A”-ReCCMSH(Arg^11^) was heated for 40 min at 40°C. Radiochemical efficiency was reported to be >95% with a specific activity of 10.6 GBq/µmol (287 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+in+vitro)]

Chen et al. (10) determined the 50% inhibition concentration (IC_50_) value of DOTA-ReCCMSH(Arg^11^) to be 1.2 ± 0.3 nM using B16/F1 murine melanoma cells with ^125^I-(Tyr^2^)-[Nle^4^, D-Phe]α-MSH (^125^I-NDP). In comparison, the IC_50_ value of ReCCMSH(Arg^11^) was 2.9 ± 0.3 nM. Wei et al. (13) found that the IC_50_ value for CHX-A”-ReCCMSH(Arg^11^) was 3.8 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+rodentia)]

Wei et al. (13) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.111 MBq (0.003 mCi, 7.3 pmol) ^111^In-CHX-A”-ReCCMSH(Arg^11^). The tumor uptake radioactivity levels were obtained at 30 min, 1 h, 2 h, 4 h, and 24 h, respectively: 4.38 ± 0.72% injected dose per gram (% ID/g), 4.59 ± 0.69% ID/g, 4.17 ± 0.94% ID/g, 3.87 ± 1.03% ID/g, and 1.35 ± 0.43% ID/g. The tumor retention was high up to 4 h after injection. Pretreatment with 9 nmol unlabeled NDP significantly reduced the tumor uptake to 1.19 ± 0.23% ID/g (P < 0.001) at 2 h after injection. No other tissues showed significant inhibition by unlabeled NDP. The ^111^In-CHX-A”-ReCCMSH(Arg^11^) uptake in nontarget tissue (except the kidneys) was low at 2 h. Furthermore, the radioactivity was quickly cleared from most of the tissues (except the kidneys) at 2 h after injection (e.g., kidney: 23.34 ± 4.46% ID/g at 30 min and 21.14 ± 6.45% ID/g at 2 h; liver: 1.74 ± 0.65% ID/g at 30 min and 0.73 ± 0.06% ID/g at 2 h; blood: 3.78 ± 2.51% ID/g at 30 min and 0.47 ± 0.22% ID/g at 2 h; lung: 4.84 ± 1.73% ID/g at 30 min and 1.59 ± 0.62% ID/g at 2 h). The tumor/muscle and tumor/blood ratios at 2 h were 38 and 9, respectively.

SPECT imaging of mice bearing the B16/F1 melanoma tumors was conducted at 2 h after intravenous injection of 13 MBq (0.35 mCi) ^111^In-CHX-A”-ReCCMSH(Arg^11^). The tumor and kidneys were clearly visible. Preinjection of 9 nmol unlabeled NDP inhibited the tumor accumulation, whereas there was little inhibition of radioactivity in the kidneys. In comparison with ^86^Y-DOTA-ReCCMSH(Arg^11^), ^111^In- and ^68^Ga-CHX-A”-ReCCMSH(Arg^11^) exhibited lower liver accumulation. ^111^In- and ^86^Y-CHX-A”-ReCCMSH(Arg^11^) showed higher tumor accumulation than ^68^Ga-CHX-A”-ReCCMSH(Arg^11^), which has a lower specific activity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+human)]

No publication is currently available.

## NIH Support

Intramural Research Program, R24 CA86307, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Wei L., Butcher C., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Lewis J.S. (2007). Synthesis and biologic evaluation of 64Cu-labeled rhenium-cyclized alpha-MSH peptide analog using a cross-bridged cyclam chelator. J Nucl Med.
12 Wei L., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Vavere A.L., Lewis J.S. (2007). Gallium-68-labeled DOTA-rhenium-cyclized alpha-melanocyte-stimulating hormone analog for imaging of malignant melanoma. Nucl Med Biol.
13 Wei L., Zhang X., Gallazzi F., Miao Y., Jin X., Brechbiel M.W., Xu H., Clifford T., Welch M.J., Lewis J.S., Quinn T.P. (2009). Melanoma imaging using 111In-, 86Y- and 68Ga-labeled CHX-A''-Re(Arg11)CCMSH. Nucl Med Biol.